# ^64^Cu-DOTA hu4D5v8 (scFv-C_H_2-C_H_3)_2_

Chemical name: | ^64^Cu-DOTA hu4D5v8 (scFv-C_H_2-C_H_3)_2_
Abbreviated name: | ^64^Cu-DOTA hu4D5v 8 scFv-Fc DM
Synonym: | ^64^Cu-Trastuzumab single-chain Fv-Fc double-mutant antibody fragment
Agent Category: | Antibody
Target: | Human epidermal growth factor receptor 2 (HER2)
Target Category: | Antibody to antigen binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal/contrast: | ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=119533), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=183984) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29)]

^64^Cu-Trastuzumab single-chain Fv-Fc double-mutant antibody fragment (^64^Cu-DOTA hu4D5v8 scFv-Fc DM), which is formed by the conjugation of ^111^In with an engineered recombinant humanized monoclonal antibody (MAb) fragment against the antigen of human epidermal growth factor receptor 2 (HER2), has been developed for imaging of human breast cancer (1, 2).

The epidermal growth factor receptors (HER/erbB) with tyrosine kinase activity are involved in transmission of signals controlling normal cell development, growth, differentiation, and survival (2-4). This cell-surface receptor family consists of four distinct members, the epidermal growth factor receptors HER1, HER2, HER3, and HER4. These receptors are found in various combinations in different tissues. There are nine ligands that bind directly to HER1, HER3, or HER4. HER2 can be activated as a result of ligand binding to other HER receptors. The ligandless HER2 receptor is encoded by the human gene HER2/c-erbB2 (HER2/neu). It has been found to be overexpressed in a wide variety of human cancers and in 20-30% of primary breast cancers (5). This overexpression is associated with aggressive tumor growth and metastatic activity. In breast cancer, HER2/neu gene amplification can result in HER2 protein levels in tumor cells that are 10- to 100-fold higher than in normal breast epithelium. HER2 overexpression is considered a negative prognostic indicator for breast cancer.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (6-8). Anti-HER2 MAbs have been generated for inhibiting the growth of tumor cells that possess activated HER2/neu receptors (9). Murine 4D5 MAb was raised against human breast and ovarian tumor cell lines overexpressing p185^HER2^. This MAb was found to recognize an extracellular epitope (amino acids 529-627) in the cysteine-rich II domain, which resides very close to the transmembrane region (9). Murine 4D5 MAb was fully humanized by Carter et al. (10) to generate the humAb4D5-8 MAb in an effort to improve the safety and tolerance of the antibody for clinical applications. Trastuzumab is of the IgG_1_ kappa class and binds to the recombinant HER2 extracellular domain with an affinity constant (K_d_) of 0.1 nM. Cardiotoxicity is the most serious complication of trastuzumab use in humans (5, 11). One potential application of a radiolabeled anti-HER2 MAb is the pretreatment imaging of breast cancer patients to predict the cardiotoxicity and therapeutic efficacy of unlabeled trastuzumab.

Molecular imaging with radiolabeled intact antibody is hampered by the relatively slow clearance of the large intact antibody (150 kDa), which contributes to a high background signal (12-14). The blood clearance of antibodies is controlled by the antibody molecular size and the Fc portion (C_H_2-C_H_3 region). This problem can be minimized by the use of smaller antibody fragments that are cleared more rapidly through the kidneys. Enzymatically produced fragments such as Fab (55 kDa) and bioengineered fragments (recombinant domain-deleted antibodies) such as single-chain Fv (scFv; 25 kDa) or various minibodies (scFv-Fc DM; 105 kDa) have been shown to be effective in producing higher tumor/blood ratios. The scFv-Fc DM ((scFv-C_H_2-C_H_3)_2_) minibody appears to have certain mutations in the Fc region that mediate Fc receptor interactions and modulate the clearance kinetics of the antibody fragment (12, 13). Various anti-HER2 MAbs have been labeled with ^131^I, ^125^I, ^111^In, ^86^Y, ^90^Y, ^64^Cu, ^76^Br, or Gd for potential imaging and therapeutic applications (1, 12, 15-20). Labeling with radiometals is generally achieved by indirect labeling with use of a bifunctional chelating agent (21, 22). ^64^Cu has a half-life (t_½_) of 12.7 h and decays 17.9% by positron emission, 37.1% by beta emission, and 45% by electron capture (23). These physical properties allow ^64^Cu to be used for positron emission tomography (PET) and therapy applications.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20synthesis)]

Assembly and production of the minibody was similar to the procedure used by Olafsen et al. (24) to prepare the scFv-C_H_3 dimer. The V genes were isolated and identified from the 10H8.C6.F12 hybridoma cell line. Splice overlap extension PCR was used to create fully synthetic variable genes. Full-length hu4D5v8 V_L_ and V_H_ chain genes were assembled into a scFv with an 18-amino-acid GlySer-rich linker (12). The scFv was then fused to the mammalian expression vector pEE12 to produce the scFv-Fc DM fragment. The anti-p185^HER2^ scFv-FC DM construct was expressed in NSO murine myeloma cells. The protein was selected in glutamine-deficient medium, screened by ELISA, analyzed by Western blot for size, and purified by dialysis and chromatography. The yield after purification was 27.3 mg/liter.

The purified protein was conjugated to the commercially available 1,4,7,10-tetrazacyclododecane-N,N´,N´´,N´´´-tetraacetic acid (DOTA) by use of the water-soluble N-hydroxysuccinimide (sulfo-NHS) method (25). In this method, N-hydroxysulfosuccinimidyl DOTA (DOTA-OSSu) was prepared by reacting sulfo-NHS and 1-ethyl-3-[3-(dimethylamino)propyl]carbodiimide with DOTA at 4 °C for 30 min. The fragment hu4D5v8 scFv-Fc DM was then reacted with DOTA-OSSu in 0.1 M Na_2_HPO_4_ (pH 7.5) at 4 °C for 24 h with continuous end-over-end mixing. The conjugate was purified by dialysis. The ^64^Cu labeling was achieved by incubating 290-440 μg of DOTA-hu4D5v8 scFv-Fc DM conjugate with 25.9-111 MBq (0.7-3 mCi) of ^64^CuCl_2_ in 0.1 M ammonium citrate (pH 5.5) for 50 min at 43 °C (12). The reaction was stopped by addition of diethylenetriaminepentaacetic acid to 1 mM ^64^Cu-DOTA-hu4D5v8 scFv-Fc. DM minibody was purified by size-exclusion high-performance chromatography. Immunoreactivity was determined by the cell binding assay with use of the human breast tumor cell line MCF7/HER2. In two radiolabeling experiments, the labeling efficiencies were 100% and 77% with immunoreactivities of 58% and 52%, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20In%20vitro)]

Using competitive binding assay with MCF7/HER2 cells, Olafsen et al. (12) determined that the relative K_D_ of hu4D5v8 scFv-Fc DM was 6.7 nM. In comparison, the K_D_ for intact trastuzumab was estimated to be 2 nM. Immunochemical staining was done in frozen sections of MCF7/HER2 tumors and kidneys from normal nude mouse. The staining patterns of the cell membrane by hu4D5v8 scFv-Fc DM and intact trastuzumab were indistinguishable.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20rodentia)]

Olafsen et al. (12) performed in vivo PET imaging of ^64^Cu-hu4D5v8 scFv-Fc DM in nude mice with s.c. implanted human breast tumor (positive HER2-expressing MCF/HER2; 1,398 ± 4 × 10^3^ receptors/cell (26)) and human breast cancer (low HER2-expressing MD-MBA-231; 115 ± 0.1 × 10^3^ receptors/cell (26)). Each mouse received 4.74-5.18 MBq (128-140 μCi) of ^64^Cu-hu4D5v8 scFv-Fc DM with a specific activity of 0.37 MBq (1.8 μCi)/μg (38.85 GBq (1.05 Ci)/μmol based on 105 kDa of hu4D5v8 scFv-Fc DM). A whole-body microPET scan was done at 3-4 and 18-21 h after injection. The values for percentage of injected dose (% ID)/g were determined from the images with use of the regions of interest (ROI) technique. After scanning, the animals were sacrificed at 21 h, and tissues were excised for in vitro assay. Imaging showed radioactivity localizations of ^64^Cu-hu4D5v8 scFv-Fc DM in both MCF/HER2 and MD-MBA-231 tumors at 4 and 21 h. For the MCF/HER2 tumors, the values for the ROI (n = 4) were estimated to be 9.0 ± 2.7 and 11.8 ± 1.0% ID/g (tumor/background ratio = 4.5:1) at 4 and 21 h, respectively. The in vitro assay at 21 h was 12.2 ± 2.4% ID/g. For the MD-MBA-231 tumors, the values for the ROI were 7.7 ± 0.8 and 8.8 ± 1.9% ID/g (tumor/background ratio = 3.4:1) at 4 and 21 h, respectively. The in vitro assay at 21 h was 7.5 ± 0.7% ID/g. The liver and kidneys were the major organs that showed radioactivity uptake. The authors of the study stated that compared with other bioengineered fragments, ^64^Cu-hu4D5v8 scFv-Fc DM showed improved tumor targeting and reduced kidney uptake.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%25)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28radiolabeled%20trastuzumab%20single-chain%20Fv-Fc%20antibody%20fragment%29%20OR%20%28anti-p185HER2%20antibody%20fragment%29%20AND%20human)]

No publication is currently available.

## NIH Support

NIH Intramural Support. NIH grants CA 43904, CA 48780, CA 86306.

## References

1 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
2 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
3 Frankel C. Development and clinical overview of trastuzumab (herceptin) Semin Oncol Nurs 2000 16Suppl 14 13 7 11151453
4 Sliwkowski M.X. Lofgren J.A. Lewis G.D. Hotaling T.E. Fendly B.M. Fox J.A. Nonclinical studies addressing the mechanism of action of trastuzumab (Herceptin) Semin Oncol 1999 26Suppl 124 60 70 10482195
5 Slamon D.J., Leyland-Jones B., Shak S., Fuchs H., Paton V., Bajamonde A., Fleming T., Eiermann W., Wolter J., Pegram M., Baselga J., Norton L. (2001). Use of chemotherapy plus a monoclonal antibody against HER2 for metastatic breast cancer that overexpresses HER2. N Engl J Med.
6 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
7 Milenic D.E., Brechbiel M.W. (2004). Targeting of radio-isotopes for cancer therapy. Cancer Biol Ther.
8 Kowalsky R.J., Falen S.W. (2004). Radiopharmaceutcals in nuclear pharmacy and nuclear medicine. Second ed. , Washington, D.C.: APhA. 733-752.
9 Fendly B.M., Winget M., Hudziak R.M., Lipari M.T., Napier M.A., Ullrich A. (1990). Characterization of murine monoclonal antibodies reactive to either the human epidermal growth factor receptor or HER2/neu gene product. Cancer Res.
10 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
11 Behr T.M., Behe M., Wormann B. (2001). Trastuzumab and breast cancer. N Engl J Med.
12 Olafsen T., Kenanova V.E., Sundaresan G., Anderson A.L., Crow D., Yazaki P.J., Li L., Press M.F., Gambhir S.S., Williams L.E., Wong J.Y., Raubitschek A.A., Shively J.E., Wu A.M. (2005). Optimizing radiolabeled engineered anti-p185HER2 antibody fragments for in vivo imaging. Cancer Res.
13 Kenanova V., Olafsen T., Crow D.M., Sundaresan G., Subbarayan M., Carter N.H., Ikle D.N., Yazaki P.J., Chatziioannou A.F., Gambhir S.S., Williams L.E., Shively J.E., Colcher D., Raubitschek A.A., Wu A.M. (2005). Tailoring the pharmacokinetics and positron emission tomography imaging properties of anti-carcinoembryonic antigen single-chain Fv-Fc antibody fragments. Cancer Res.
14 Xu X., Clarke P., Szalai G., Shively J.E., Williams L.E., Shyr Y., Shi E., Primus F.J. (2000). Targeting and therapy of carcinoembryonic antigen-expressing tumors in transgenic mice with an antibody-interleukin 2 fusion protein. Cancer Res.
15 Blend M.J., Stastny J.J., Swanson S.M., Brechbiel M.W. (2003). Labeling anti-HER2/neu monoclonal antibodies with 111In and 90Y using a bifunctional DTPA chelating agent. Cancer Biother Radiopharm.
16 Winberg K.J., Persson M., Malmstrom P.U., Sjoberg S., Tolmachev V. (2004). Radiobromination of anti-HER2/neu/ErbB-2 monoclonal antibody using the p-isothiocyanatobenzene derivative of the [76Br]undecahydro-bromo-7,8-dicarba-nido-undecaborate(1-) ion. Nucl Med Biol.
17 Xu F.J., Yu Y.H., Bae D.S., Zhao X.G., Slade S.K., Boyer C.M., Bast R.C., Zalutsky M.R. (1997). Radioiodinated antibody targeting of the HER-2/neu oncoprotein. Nucl Med Biol.
18 Palm S., Enmon R.M., Matei C., Kolbert K.S., Xu S., Zanzonico P.B., Finn R.L., Koutcher J.A., Larson S.M., Sgouros G. (2003). Pharmacokinetics and Biodistribution of (86)Y-Trastuzumab for (90)Y dosimetry in an ovarian carcinoma model: correlative MicroPET and MRI. J Nucl Med.
19 Tsai S.W., Sun Y., Williams L.E., Raubitschek A.A., Wu A.M., Shively J.E. (2000). Biodistribution and radioimmunotherapy of human breast cancer xenografts with radiometal-labeled DOTA conjugated anti-HER2/neu antibody 4D5. Bioconjug Chem.
20 Kobayashi H., Shirakawa K., Kawamoto S., Saga T., Sato N., Hiraga A., Watanabe I., Heike Y., Togashi K., Konishi J., Brechbiel M.W., Wakasugi H. (2002). Rapid accumulation and internalization of radiolabeled herceptin in an inflammatory breast cancer xenograft with vasculogenic mimicry predicted by the contrast-enhanced dynamic MRI with the macromolecular contrast agent G6-(1B4M-Gd)(256). Cancer Res.
21 Fritzberg A.R., Berninger R.W., Hadley S.W., Wester D.W. (1988). Approaches to radiolabeling of antibodies for diagnosis and therapy of cancer. Pharm Res.
22 Hnatowich D.J., Childs R.L., Lanteigne D., Najafi A. (1983). The preparation of DTPA-coupled antibodies radiolabeled with metallic radionuclides: an improved method. J Immunol Methods.
23. Schlyer, D.J., Production of radionuclides in accelerators, in Handbook of Radiopahrmaceuticals, Radiochemistry and Applications, M.J. Welch and C.S. Redvanly, Editors. 2003, John Wiley & Sons Inc.: Hoboken, New Jersey. p. 1-71.
24 Olafsen T., Tan G.J., Cheung C.W., Yazaki P.J., Park J.M., Shively J.E., Williams L.E., Raubitschek A.A., Press M.F., Wu A.M. (2004). Characterization of engineered anti-p185HER-2 (scFv-CH3)2 antibody fragments (minibodies) for tumor targeting. Protein Eng Des Sel.
25 Lewis M.R., Kao J.Y., Anderson A.L., Shively J.E., Raubitschek A. (2001). An improved method for conjugating monoclonal antibodies with N-hydroxysulfosuccinimidyl DOTA. Bioconjug Chem.
26 Aguilar Z., Akita R.W., Finn R.S., Ramos B.L., Pegram M.D., Kabbinavar F.F., Pietras R.J., Pisacane P., Sliwkowski M.X., Slamon D.J. (1999). Biologic effects of heregulin/neu differentiation factor on normal and malignant human breast and ovarian epithelial cells. Oncogene.